# [^99m^Tc]Anti-CD3 monoclonal antibody

Chemical name: | [^99m^Tc]Anti-CD3 monoclonal antibody
Abbreviated name: | [^99m^Tc]Anti-CD3 mAb
Synonym: | ^99m^Tc-OKT3
Agent Category: | Monoclonal antibody
Target: | CD3 antigen on human T cells
Target Category: | Antibody-ligand binding
Method of detection: | Single-photon emission computed tomography (SPECT) or gamma planar imaging
Source of signal: | ^99m^Tc
Activation: | No
Studies: | - Humans | .

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+OKT3&WebEnv=0LDqyW8YezKYPS53viZ-u0X4sRwxDX_nvCL46q0TjWbfWmFEl_odftIiU6yaV81MFqnK6Dzn2ii4dEb%407748428072881B60_0000SID&WebEnvRq=1)]

A characteristic feature of rheumatoid arthritis (RA) is progressive inflammation and proliferation of the synovium in the joints, but the disease may also have extra-articular manifestations (1, 2). The inflammatory response observed during RA is believed to be caused by the presence of CD4^+^ and CD8^+^ T lymphocytes in the RA-inflamed tissue, which indicates that these cells may play an important role in the pathogenesis of this disease (3). Although radiography, scintigraphy, ultrasonography, and magnetic resonance imaging with examination both before and after contrast administration are used for detecting early arthritis, none of these imaging procedures can adequately measure the state of or detect the early signs of arthritis in the tissue (4). The use of radiopharmaceuticals to detect RA has also been explored, but these bone-seeking agents accumulate nonspecifically in the arthritic joint, depicting bone metabolism rather than inflammation of the synovium (5, 6).

Because T cells are known to accumulate in the inflamed tissue during RA, the possible use of monoclonal antibodies (mAb) directed against membrane-surface molecules on T cells to detect, evaluate, and monitor the disease has been explored (7-10). Among these mAbs, the anti-CD3 antibody is directed against the CD3 antigen present on the T cells and is widely used as an immunosuppressive drug in organ transplant patients (11). This mAb is approved (http://www.orthobiotech.com/common/prescribing_information/OKT3/PDF/OKT3_PI.pdf) by the United States Food and Drug Administration for the reversal of acute renal, cardiac, or hepatic allograft rejections and is in clinical trials (http://clinicaltrials.gov/ct2/results?term=OKT3) for the treatment of a variety of conditions involving T cells; it is available commercially. Investigators have evaluated the use of a metastable technetium (^99m^Tc)-labeled anti-CD3 mAb ([^99m^Tc]anti-CD3 mAb or [^99m^Tc]OKT3) for the detection of acute renal rejection in transplant patients and also for monitoring RA synovitis (7, 9, 10).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+OKT3+synthesis&WebEnv=0vzdWffN4y9fddN3AFcXzOSf_Q4tGN_knzwV_mcOr2nB67Q1AcVVU-mW0hH7Q0D06NOaqAQ9dEsEfo8%407748428072881B60_0000SID&WebEnvRq=1)]

The source of OKT3 used for the imaging work was not mentioned in the publication (9, 10). The labeling of OKT3 was described by Martins et al. (10). Briefly, the mAb was incubated with 2-mercaptoethanol for 10 min along with an exogenous chelator; the nature of the chelator was not described. Stannous chloride was added to the mAb solution, and the mixture was incubated for another 10 min. Subsequently, ^99m^Tc as sodium pertechnetate was added to the mixture and incubated for 20 min (incubation temperature was not provided). After the labeling reaction, the mAb was filtered through a 0.45-micron filter to remove any colloidal form of [^99m^Tc]OKT3. The investigators claimed that >90% of the mAb was labeled with ^99m^Tc (10). The stability and specific activity of the labeled mAb were not provided (10).

Marcus et al described a different method for the generation of [^99m^Tc]OKT3 (7). The commercial antibody was first incubated with ascorbic acid for the reduction of one or two disulphide bonds in the mAb. The conditions (time and temperature) for this incubation were not provided. The reaction mixture was then mixed with sodium pertechnetate previously reduced with sodium hydrosulphite and incubated for 30 min. Unbound ^99m^Tc was separated from the labeled mAb by centrifugation in a Centricon 30 microconcentrator. The radiochemical yield of the reaction was >95%, and the colloid formation was consistently <5% as determined by thin-paper chromatography and high-performance liquid chromatography on a Water’s protein pak SW 300 column. The stability and specific activity of the labeled product were not provided (7).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+OKT3+in+vitro&WebEnv=03gnu9_gXr8YWPnJ9HDgglR1T3hk2Klus7GIj6eA39jPGg79gM7XcpTa600SEe-4U1sJMOtWeU7e1qP%407748428072881B60_0000SID&WebEnvRq=1)]

No references are currently available.

## Animal Studies

### Rodents

[PubMed] (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+OKT3+rodentia&WebEnv=06HK32GhRoLbG5DMvTtVNIKnQfiwbvv9qrtP3TxtaGfJfU1zWUCAt3hu4SSo5gMLo-Gav860PihLc2j%407748428072881B60_0000SID&WebEnvRq=1)

No references are currently available.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+OKT3+non+primate+mammals&WebEnv=0wHOiJurKE00tfBdkRS2HC5Pf3F7QAHENfntTSq-5VKWpXQMHwIDSoaYf-pN7fzSTtztIl98viLY80v%407748428072881B60_0000SID&WebEnvRq=1)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+OKT3+non+human+primates&WebEnv=02rY_2OrsvG_1USvZH1HPT2SepLpcc0gB3p9QjeaMmRXoanqy6-E02rfOSakTaliXzAfs02ZTGpUhWX%407748428072881B60_0000SID&WebEnvRq=1)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

The use of [^99m^Tc]OKT3 scintigraphy to diagnose acute rejection in renal transplants was evaluated by Martins et al. (10). Among the 22 renal transplant patients in this study, an increased kidney uptake of [^99m^Tc]OKT3 was observed with time in 3 patients experiencing allograft rejection. A histopathological examination of the kidneys in these 3 patients confirmed the observations made with [^99m^Tc]OKT3 scintigraphy. The investigators reported that a larger number of kidney transplant patients were being monitored with this technique to confirm the use of [^99m^Tc]OKT3 to detect kidney allograft rejection.

In another study, [^99m^Tc]OKT3 was given intravenously to seven RA and two psoriatic arthritis patients to evaluate the use of this labeled mAb for the identification of an inflamed synovium (7). Specific regional imaging and anterior and posterior whole-body scans were performed on the patients 20 min after administration of the labeled mAb. Based on criteria for the classification of RA specified by the American College of Rheumatology, patients with asymptomatic and joints with mild pain or minimal tenderness showed normal uptake of the label. Patients who described moderate to severe pain in their joints showed moderate to marked increases in radioactivity uptake. With these results the investigators concluded that [^99m^Tc]OKT3 could possibly be used to measure the effectiveness of a treatment for RA and other conditions that result in an inflamed synovium (7).

Martins et al. investigated the use of [^99m^Tc]OKT3 to monitor RA in 38 patients (9). Planar anterior images of the patients' wrists, metacarpophalangeal and interphalangeal joints, elbows, shoulders, and knees were obtained 1 h and 3 h after administration of [^99m^Tc]OKT3. A significant correlation (P < 0.05) between the accumulation of [^99m^Tc]OKT3 and swollen or tender joints and the visual analog scale was reported. The investigators observed no correlation between the accumulation of radioactivity and the patients' age, gender, duration of disease, and erythrocyte sedimentation rate. From these results the investigators concluded that [^99m^Tc]OKT3 scintigraphy was a reliable and objective method to detect synovial activity, and this technique could possibly be used to observe disease prognosis.

## Supplemental Information

[Disclaimers]

## NIH Support

Some of the studies presented in this chapter were funded by NIH grant (MLT)CA-51960.

## References

1 Goldring M.B., Goldring S.R. (2007). and , Osteoarthritis.
2 Goekoop Y.P., Allaart C.F., Breedveld F.C., Dijkmans B.A. (2001). Combination therapy in rheumatoid arthritis. Curr Opin Rheumatol.
3 Breedveld F.C., Verweij C.L. (1997). T cells in rheumatoid arthritis. Br J Rheumatol.
4 Backhaus M., Burmester G.R., Sandrock D., Loreck D., Hess D., Scholz A., Blind S., Hamm B., Bollow M. (2002). Prospective two year follow up study comparing novel and conventional imaging procedures in patients with arthritic finger joints. Ann Rheum Dis.
5 van der Heijde D.M., van 't Hof M., van Riel P.L., van de Putte L.B. (1993). Validity of single variables and indices to measure disease activity in rheumatoid arthritis. J Rheumatol.
6 Kraus V.B. (1997). Pathogenesis and treatment of osteoarthritis. Med Clin North Am.
7 Marcus C., Thakur M.L., Huynh T.V., Louie J.S., Leibling M., Minami C., Diggles L. (1994). Imaging rheumatic joint diseases with anti-T lymphocyte antibody OKT-3. Nucl Med Commun.
8 Kinne R.W., Becker W., Schwab J., Schwarz A., Kalden J.R., Emmrich F., Burmester G.R., Wolf F. (1994). Imaging rheumatoid arthritis joints with technetium-99m labelled specific anti-CD4- and non-specific monoclonal antibodies. Eur J Nucl Med.
9 Martins F.P., Gutfilen B., de Souza S.A., de Azevedo M.N., Cardoso L.R., Fraga R., da Fonseca L.M. (2008). Monitoring rheumatoid arthritis synovitis with 99mTc-anti-CD3. Br J Radiol.
10 Martins F.P., Souza S.A., Goncalves R.T., Fonseca L.M., Gutfilen B. (2004). Preliminary results of [99mTc]OKT3 scintigraphy to evaluate acute rejection in renal transplants. Transplant Proc.
11 Ortho B. (2004). Orthoclone OKT3 sterile solution, Ortho Biotech: Raritan, NJ.